# Anti-malondialdehyde-modified low-density lipoprotein MDA2 monoclonal antibody gadolinium-labeled micelles

Chemical name: | Anti-malondialdehyde-modified low-density lipoprotein MDA2 monoclonal antibody gadolinium-labeled micelles
Abbreviated name: | MDA2 micelles
Synonym:
Agent category: | Antibody
Target: | Malondialdehyde-modified low-density lipoprotein (MDA-LDL)
Target category: | Antigen
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=44888831), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=217035086) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=338) for more information about apolipoprotein B.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T_2_ primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Apolipoprotein E (apoE) is essential for the normal catabolism of triglyceride-rich lipoprotein chylomicrons (lipoprotein particles) (2). Oxidation of low-density lipoprotein (LDL) generates a number of highly reactive short chain-length aldehydic fragments of oxidized fatty acids capable of conjugating with lysine residues of apoliprotein B and other proteins. Oxidized LDL is present in atherosclerotic lesions and is essential for formation of foam cells in atherosclerotic plaques. During atherogenic conditions, depositions of lipids and extracellular matrix proteins on the endothelial cell surfaces of the aorta and cells lead to the development of atherosclerotic plaques (3), which may erode and rupture. MDA2 is a murine monoclonal antibody to malondialdehyde-lysine epitopes of MDA-LDL and other oxidatively modified proteins but not to normal LDL (4). Briley-Saebo et al. (5) studied magnetic resonance imaging of atherosclerotic lesions in mice using micelles containing Gd and MDA2.

### Related Resource Links:

- Chapters in MICAD (MDA (http://www.ncbi.nlm.nih.gov/books?term=malondialdehyde%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Apolipoprotein E (http://www.ncbi.nlm.nih.gov/gene/348))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Apolipoprotein E (http://omim.org/entry/107741))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+synthesis)]

1,2-Distearoyl-sn-glycer-3-phosphoethanolamine-n-methoxy(polyethylene glycol-2000) ammonium salt (PEG-DSPE), Gd-DTPA-bis(stearyl-amid), and PEG-malamide-DSPE were dissolved at a molar ratio of 49:50:1 in a chloroform:methanol solution with rhodamine added as a fluorescent label (5). The solvents were removed under heat and vacuum until a thin film was formed. The film was hydrated in a HEPES buffer (pH 7.0), and the sample was incubated at 65°C until micelles formed. MDA2 was modified with S-acetylthioglycolic acid N-hydroxysuccinimide ester and then covalently linked to the surface of the Gd micelles. Gd-MDA2 micelles have a hydrated diameter of 22 ± 2 nm with an r1 value of 9.3 nM^-1^s ^-1^ at 60 MHz and 40ºC. Neither the number of Gd molecules nor MDA2 monoclonal antibodies per micelle was reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+in+vitro)]

^125^I-MDA2 has been shown to bind specifically to human MDA-LDL but not to normal human LDL, high-density lipoprotein, very low-density lipoprotein, or bovine serum albumin (6). Confocal microscopy analysis showed that the highest accumulation of MDA2 micelles in macrophages was obtained when both the macrophages and MDA2 micelles were pretreated with MDA-LDL than either one alone (5). The Gd contents were 0.3 µg/ml for macrophages and MDA2 micelles with no pre-exposure, 0.5 µg/ml for macrophages pretreated with MDA-LDL, 11 µg/ml for MDA2 micelles pretreated with MDA-LDL, and 15 µg/ml for both macrophages and MDA2 micelles pretreated with MDA-LDL, respectively. The enhanced uptake as in the latter two cases may be due to uptake of MDA-LDL MDA2 micelle complexes by macrophages.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+rodentia)]

Briley-Saebo et al. (5) performed ex vivo biodistribution studies of MDA2 micelles in 11-month-old apoE^-/-^ knockout mice that were fed a high-fat, high-cholesterol diet for 6 weeks. Animals were injected with either 0.075 mmol Gd/kg MDA2 micelles (n = 8 mice) or IgG micelles (n = 3 mice). The accumulation of Gd was determined as percent of injected dose (% ID) at 24, 48, and 96 h after injection. The blood half-life was 14.3 h for MDA2 micelles and 1.4 h for IgG micelles, whereas the blood half-life was ~1.5 h for both micelles in the wild-type mice. Liver, spleen, and kidney uptake peaked at 48 h with 38% ID, 6% ID, and 2% ID of Gd, respectively. Accumulation was <0.4% ID in the heart and lung. The abdominal lymph nodes showed 10, 80, and 37 µg/g Gd at 24, 48, and 96 h, respectively. The atherosclerotic aorta showed 0.30, 0.48, and 0.12% ID at 24, 48, and 96 h, respectively. No Gd was detected in the aorta after injection of either the untargeted or IgG micelles. Sequential T1-weighted MRI images (9.4 T) showed that MDA2 micelles caused increased atherosclerotic arterial vessel wall enhancement at 24–72 h after injection. The mean enhancement was 60%, 90%, and 125% at 24, 48, and 72 h, respectively. In contrast, IgG and untargeted micelles caused minimal signal enhancement. The liver showed enhancement of 33% with MDA2 micelles at the three time points. Pretreatment with excess MDA2 reduced the enhancement to 20% in the aorta and -8% in the liver at 72 h. Confocal microscopy revealed that MDA2 colocalized primarily with CD68 staining (macrophages) in the arterial wall.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+human)]

No publication is currently available.

## NIH Support

R01 HL071021, R01 HL078667

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Eichner J.E., Dunn S.T., Perveen G., Thompson D.M., Stewart K.E., Stroehla B.C. (2002). Apolipoprotein E polymorphism and cardiovascular disease: a HuGE review. Am J Epidemiol.
3 Libby P., Ridker P.M., Maseri A. (2002). Inflammation and atherosclerosis. Circulation.
4 Palinski W., Yla-Herttuala S., Rosenfeld M.E., Butler S.W., Socher S.A., Parthasarathy S., Curtiss L.K., Witztum J.L. (1990). Antisera and monoclonal antibodies specific for epitopes generated during oxidative modification of low density lipoprotein. Arteriosclerosis.
5 Briley-Saebo K.C., Shaw P.X., Mulder W.J., Choi S.H., Vucic E., Aguinaldo J.G., Witztum J.L., Fuster V., Tsimikas S., Fayad Z.A. (2008). Targeted molecular probes for imaging atherosclerotic lesions with magnetic resonance using antibodies that recognize oxidation-specific epitopes. Circulation.
6 Tsimikas S., Palinski W., Halpern S.E., Yeung D.W., Curtiss L.K., Witztum J.L. (1999). Radiolabeled MDA2, an oxidation-specific, monoclonal antibody, identifies native atherosclerotic lesions in vivo. J Nucl Cardiol.